# 2’-[^18^F]Fluoroflumazenil

Chemical name: | [^18^F]fluoroethyl 8-fluoro-5-methyl-6-oxo-5,6-dihydro-4H-benzo-[f]imidazo[1,5-a][1,4]diazepine-3-carboxylate
Abbreviated name: | [^18^F]FFMZ
Synonym: | 2’-[^18^F]fluoroflumazenil; 3-(2’-[^18^F]fluoro-FMZ)
Agent Category: | Compound
Target: | Benzodiazepine receptor
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D)]

Benzodiazepines are used for their sedative, anxiolytic, and muscle-relaxant properties. Their mechanism of action involves the binding of a ligand to a specific benzodiazepine receptor. Alteration of the central benzodiazepine receptor (CBR) has been reported in various diseases and pathologic conditions such as Alzheimer’s disease, epilepsy, or cerebral ischemia (1-4).

CBRs have been studied in vivo by positron emission tomography (PET) and single photon emission computed tomography, and the existence of a specific benzodiazepine receptor linked to the γ-aminobutyric acid (GABA) receptor/chloride ionophore has been shown by use of diazepam (4).

[^11^C]Flumazenil, a highly selective benzodiazepine antagonist, has been the most widely used agent for PET imaging of CBRs, but the short half-life of ^11^C (20 min) limits its use. To overcome this great disadvantage, the flumazenil analog [^18^F]fluoroethyl 8-fluoro-5-methyl-6-oxo-5,6-dihydro-4H-benzo-[f]imidazo[1,5-a][1,4]diazepine-3-carboxylate ([^18^F]fluoroflumazenil; [^18^F]FFMZ) has been developed and is currently under study. It can be conveniently synthesized and labeled, and preliminary research shows some favorable specific binding properties for CBRs.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

A one-pot, one-step synthesis method for [^18^F]FFMZ was developed by Yoon et al. (5). In that procedure, the two precursors 2´-tosyloxyflumazenil (TFMZ) and 2´-mesyloxyflumazenil (MFMZ) were synthesized in three steps, labeled with no-carrier-added [^18^F]fluoride, and then activated by repeated azeotropic distillation with Kryptofix 2.2.2./potassium carbonate in acetonitrile (MeCN).

An automated process for the labeling and purification of [^18^F]FFMZ was also developed by Yoon et al. (5). This process involved adding 10 mg of the precursor TFMZ or MFMZ (in 2.5 ml of MeCN) to dry [^18^F]fluoride (produced with ^18^O-enriched (>95%) water)), and heating the mixture at 85°C for 12 min while purging with He. Purification was obtained by successive filtrations through polyvinylidene difluoride filters and high-performance liquid chromatography (HPLC), with gradient elution of [^18^F]FFMZ taking 24.4 min (flow rate 5 ml/min). The entire automated procedure (after production of [^18^F]fluoride) took 97 min.

The highest labeling efficiency was obtained with 4 mg of TMZ at 110°C for 10 min; the obtained specific activity of [^18^F]FFMZ was 5.92 × 10^9^ MBq/mol (1.6 x 10^5^ Ci/mol). The reported labeling efficiency and radiochemical purity of [^18^F]FFMZ after synthesis by the automated system were 68% and 98%, respectively. Stability tests performed by Yoon et al. (5) showed that 98% of the produced [^18^F]FFMZ was intact at 37°C in human serum after 1 h.

Chang et al. (6) synthesized [^18^F]FFMZ, using a procedure similar to the one described previously by Yoon et al. (5). The radiochemical purity and specific activity (determined by analytical HPLC) reported by Chang et al. (6) were >98% and approximately 4.5 × 10^9^ MBq/mol (1.2 x 10^8^ mCi/mol), respectively.

Mitterhauser et al. (7) synthesized [^18^F]FFMZ by reaction of 3-desethylflumazenil with 2-bromo-1-[^18^F]lfuoroethane. They reported a radiopurity of [^18^F]FFMZ >98%. When starting with 52 ± 8 GBq of [^18^F]fluoride, they obtained 52.3 GBq for [^18^F]FFMZ. Specific radioactivity exceeded 89.4 GBq/µmol (2418.9 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20in%20vitro)]

An assessment of the in vitro stability of [^18^F]FFMZ in rat and human sera was made by Chang et al. (6). The experimental procedure involved incubating 25 µl of rat serum or 325 µl of human serum for 1 h in CO_2_ at 37°C. After addition of absolute ethanol (775 µl) to precipitate serum proteins, the mixture was centrifuged for 5 min at 3000 rpm, and the supernatant was analyzed by HPLC. Results showed that, in rat serum, [^18^F]FFMZ was hydrolyzed to FFMZ acid and [^18^F]fluoroethanol, with 39% of [^18^F]FFMZ degraded to [^18^F]fluoroethanol at 10 min and only 8% of [^18^F]FFMZ intact at 60 min. [^18^F]FFMZ appeared to be stable at least for 1 h in the case of human serum.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

Mitterhauser et al. (7) evaluated the biological activity of [^18^F]FFMZ with respect to the GABA(A) receptor, using male Sprague-Dawley rats/Him:OFA. Biodistribution studies were performed by injecting 1.58-2.72 MBq (4.3-7.3 × 10^-2^ mCi) of [^18^F]FFMZ (in 180-225 µl of physiologic phosphate buffer) into the tail vein. After sacrifice at 5, 15, 30, and 60 min post injection, organs were weighed and counted.

The organ showing the highest uptake of [^18^F]FFMZ was the pituitary gland (0.95 ± 0.35% injected dose (ID)/g at 15 min), followed by the cortex (0.73 ± 0.07% ID/g at 5 min) and the liver (0.70 ± 0.11% ID/g at 60 min). The lowest uptake was observed in the femur (0.35 ± 0.02% ID/g at 5 min and 0.36 ± 0.05% ID/g at 60 min), reflecting low levels of fluoride accumulation and showing that [^18^F]FFMZ is metabolically stable. The tissue/blood ratio for the whole brain was 1.46. In comparison, the ratio for [^18^F]fluoroethylflumazenil ([^18^F]FEFMZ) in previous studies was 0.73 (8). Peak uptake was obtained at 5 min post injection for all sampled brain regions. Those results showed a kinetic process comparable to the one observed for [^18^F]FEFMZ, but much faster than for [^11^C]FFMZ (9).

Ex vivo studies using a similar experimental protocol were performed by Yoon et al. (5). [^18^F]FFMZ (518 MBq (14 mCi); 0.35 ml) was injected intravenously into Sprague-Dawley rats. Receptor-blocking studies were performed with cold flumazenil (0.33 µmol; 0.3 ml). Phosphoimaging of the rat brain showed high uptake in the cortex, thalamus, and hippocampus, but those uptakes were blocked by pre-injection of cold flumazenil.

Biodistribution studies using male ICR mice have also been reported in the literature (6). The animals were sacrificed at 10, 30, and 60 min after an intravenous injection of 0.37 MBq (0.01 mCi) of [^18^F]FFMZ. Results showed a relatively uniform distribution among organs (between 2 and 3% ID/g), including the heart, lung, spleen, and muscle. Maximum uptakes for the intestine (5.7% ID/g) and bone (3.6% ID/g) were reported at 60 min post injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%20AND%20%28dog%20OR%20sheep%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%20AND%20%28primate%20NOT%20human%29)]

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%20AND%20human)]

The only human experiment reported to date was performed by Chang et al. (6), using a healthy human volunteer (age 47 years; no medication at the time of the study). After intravenous injection of 370 MBq (10 mCi) of [^18^F]FFMZ, static PET image acquisition was performed for a post-injection time period of 20 to 60 min. High uptakes in the frontal cortex, temporal cortex, occipital cortex, cerebellum, parietal cortex, and thalamus were observed (decreasing order). On the other hand, the brain stem showed low uptake of the tracer. Those results appeared to match known relative benzodiazepine receptor densities for humans.

## References

1 Marczynski TJ. (1995). GABAergic deafferentation hypothesis of brain aging and Alzheimer's disease; pharmacologic profile of the benzodiazepine antagonist, flumazenil. Rev Neurosci.
2 Thomas RJ. (1997). Seizures and epilepsy in the elderly. Arch Intern Med.
3 Nutt DJ, Malizia AL. (2001). New insights into the role of the GABA(A)-benzodiazepine receptor in psychiatric disorder. Br J Psychiatry.
4 Mohler H, Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
5 Yoon YH, Jeong JM, Kim HW, Hong SH, Lee YS, Kil HS, Chi DY, Lee DS, Chung JK, Lee MC. (2003). Novel one-pot one-step synthesis of 2'-[(18)F]fluoroflumazenil (FFMZ) for benzodiazepine receptor imaging. Nucl Med Biol.
6 Chang YS, Jeong JM, Yoon YH, Kang WJ, Lee SJ, Lee DS, Chung JK, Lee MC. (2005). Biological properties of 2'-[18F]fluoroflumazenil for central benzodiazepine receptor imaging. Nucl Med Biol.
7 Mitterhauser M, Wadsak W, Wabnegger L, Mien LK, Togel S, Langer O, Sieghart W, Viernstein H, Kletter K, Dudczak R. (2004). Biological evaluation of 2'-[18F]fluoroflumazenil ([18F]FFMZ), a potential GABA receptor ligand for PET. Nucl Med Biol.
8 Leveque P, Labar D, Gallez B. (2001). Biodistribution, binding specificity and metabolism of [18F]fluoroethylflumazenil in rodents. Nucl Med Biol.
9 Grunder G, Siessmeier T, Lange-Asschenfeldt C, Vernaleken I, Buchholz HG, Stoeter P, Drzezga A, Luddens H, Rosch F, Bartenstein P. (2001). [18F]Fluoroethylflumazenil: a novel tracer for PET imaging of human benzodiazepine receptors. Eur J Nucl Med.